# ^99m^Tc-Hydrazinonicotinamide-aminohexanoic acid-Lys^40^-exendin-4

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-aminohexanoic acid-Lys^40^-exendin-4
Abbreviated name: | [Lys^40^(Ahx-HYNIC-^99m^Tc)NH_2_]-exendin-4
Synonym: | ^99m^Tc-HYNIC-Ahx-Lys^40^-exendin-4
Agent category: | Peptide
Target: | Glucagon-like peptide-1 receptor (GLP-1R)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=248418), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&val=1916066) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=14526) for more information about exendin-4.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ahx%20Exendin-4)]

Glucagon-like peptide-1 (GLP-1, 30 amino acids) is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). GLP-1 plays an important role in glucose metabolism and homeostasis. It inhibits gastric emptying, glucagon secretion, and glucose production (2). In addition, it induces insulin release from the pancreatic β-cells as well as their proliferation. The GLP-1 receptor has been identified in normal tissues such as the pancreas, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1 receptor density is considerably greater, and the GLP-1 receptor is more frequently observed than somatostatin receptors.

Exendin-4 is a GLP-1 analog with 39 amino acids isolated from the venom of the Gila monster (Heloderma suspectum) (4). Exendin-4 and GLP-1 share a 53% amino acid sequence homology. Exendin-4 is a more potent and longer-lasting GLP-1 receptor agonist than GLP-1. Exendin-4 is resistant to cleavage by dipeptidyl peptidase IV, whereas the first two N-terminal amino acids of GLP-1 are rapidly cleaved. Exenatide, a synthetic version of exendin-4, is the first GLP-1 mimetic recently approved by the United States Food and Drug Administration (FDA) for use in select patients with type 2 diabetes (5). ^99m^Tc-Hydrazinonicotinamide-aminohexanoic acid-Lys^40^-exendin-4 ([Lys^40^(Ahx-HYNIC-^99m^Tc)NH_2_]-exendin-4) is being developed for single-photon emission computed tomography (SPECT) imaging of the GLP-1 receptor (6).

### Related Resource Links:

- Chapters in MICAD (GLP-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GLP-1R (http://omim.org/entry/138032))
- Clinical trials (Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (Exendin (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ahx%20Exendin-4%20and%20synthesis)]

The structure and composition of [Lys^40^(Ahx-HYNIC)NH_2_]-exendin-4 was verified with high-performance liquid chromatography and matrix-assisted laser desorption-ionization mass spectrometry (6). A mixture of EDDA and 370 MBq (10 mCi) ^99m^TcO_4_− was added to a vial containing tricine, SnCl_2_, and [Lys^40^(Ahx-HYNIC)NH_2_]-exendin-4 (7.7 nmol) and incubated for 10 min at 95°C, with a 95% labeling yield of [Lys^40^(Ahx-HYNIC-^99m^Tc)NH_2_]-exendin-4 and a specific activity of 48 GBq/µmol (1.3 Ci/µmol). The stability of [Lys^40^(Ahx-HYNIC-^99m^Tc)NH_2_]-exendin-4 in solution was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ahx%20Exendin-4%20and%20in%20vitro)]

Wild et al. (6) reported that [Lys^40^(Ahx-HYNIC-^99m^Tc)NH_2_]-exendin-4 was accumulated into β-cell tumors in culture with 1.50 ± 0.49% of incubation dose at 1 h and 6.50 ± 1.94% at 4 h. Most of the accumulated radioactivity was internalized into the cells (>80%).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ahx%20Exendin-4%20and%20rodentia)]

Wild et al. (6) performed ex vivo biodistribution studies with the use of Rip1Tag2 mice (n = 6/group) with spontaneous insulinoma β-cell tumors. The organ with the highest uptake was the tumor (93.1 ± 19.9% injected dose/g (% ID/g)), followed by the kidneys (60 ± 12% ID/g), lungs (16 ± 6% ID/g), pancreas (7.4 ± 2.2% ID/g), stomach (1.2 ± 0.3% ID/g), liver (0.7 ± 0.2% ID/g), and spleen (0.5 ± 0.2% ID/g) at 4 h after injection of [Lys^40^(Ahx-HYNIC-^99m^Tc)NH_2_]-exendin-4 (10 pmol/mouse). Excess unlabeled [Lys^40^(Ahx-HYNIC)NH_2_]-exendin-4 (5 nmol) blocked accumulation by >95% in the tumor and GLP-1R-expressing organs, such as the pancreas and lung, but there was little inhibition in the kidneys. Blood clearance was fast, with 0.4% ID/g remaining in the blood 4 h after injection. In contrast, the tumor washout rate was slow. The tumor/blood ratio was 29 at 0.5 h and 266 at 4 h. The tumor/muscle, tumor/pancreas, and tumor/kidney ratios were 547, 13, and 2 at 4 h, respectively.

Pinhole SPECT imaging of two Rip1Tag2 mice identified high uptake in the kidneys at 4 h after injection of 37 MBq (1 mCi) [Lys^40^(Ahx-HYNIC-^99m^Tc)NH_2_]-exendin-4 (6). SPECT images clearly identified four tumors (1.0–3.2 mm) in the pancreas in one of the mice. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ahx%20Exendin-4%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ahx%20Exendin-4%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ahx%20Exendin-4%20and%20human)]

No publication is currently available.

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Meier J.J., Nauck M.A. (2005). Glucagon-like peptide 1(GLP-1) in biology and pathology. Diabetes Metab Res Rev.
5 Nielsen L.L., Young A.A., Parkes D.G. (2004). Pharmacology of exenatide (synthetic exendin-4): a potential therapeutic for improved glycemic control of type 2 diabetes. Regul Pept.
6 Wild D., Wicki A., Mansi R., Behe M., Keil B., Bernhardt P., Christofori G., Ell P.J., Macke H.R. (2010). Exendin-4-based radiopharmaceuticals for glucagonlike peptide-1 receptor PET/CT and SPECT/CT. J Nucl Med.